# Cy5.5-Gly-His-Pro-Gly-Gly-Pro-Gln-Gly-Lys(Fitc)-Cys-Poly-L-lysine-methoxypolyethylene glycol

Chemical name: | Cy5.5-Gly-His-Pro-Gly-Gly-Pro-Gln-Gly-Lys(Fitc)-Cys-Poly-L-lysine-methoxypolyethylene glycol
Abbreviated name: | Cy5.5-GHPGGPQK(Fitc)C-PL-MPEG, Cy5.5-CatK-PGC
Synonym: | Cy5.5-GHPGGPQK(Fitc)C-Poly-L-lysine-methoxypolyethylene glycol
Agent Category: | Peptide
Target: | Cathepsin K
Target Category: | Enzyme binding
Method of detection: | Optical, Near-Infrared fluorescence
Source of signal: | Cy5.5
Activation: | Yes
Studies: | - In vitro; - Rodents | Click on cathepsin K (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=55959090) for protein information.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Poly-L-lysine+MPEG)]

Optical fluorescence imaging is increasingly used to study biological functions of specific targets (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have a wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging in small animals.

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (3). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (4). Invasive tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (5).

Several families of proteases are involved in atherogenesis, myocardial infraction, angiogenesis, and tumor invasion and metastasis (6-9). The cysteine proteases (cathepsin B, H, K, and L) and serine protease (cathepsin D) are present in the endosomal system of cells such as macrophages, epithelial cells, and tumor cells. These proteases participate in degradation of ECM and remodeling of tissues. A synthetic protected graft copolymer (PGC) consisting of poly-L-lysine (PL) with multiple methoxypolyethylene glycol (MPEG) side chains has been used as a drug carrier with efficient accumulation in tumor (10, 11). The peptide GHPGGPQKC was found to be a cathepsin K (CatK) substrate and is cleaved between Gly (G) and Gly (G) residues (12). Jaffer et al. (13) used this sequence with linking residues GHPGGPQK(Fitc)C with a Cy5.5 NIR dye molecule to attach to the unmodified PL side chains of the PGC to form a fluorescence-quenched polymer, Cy5.5-GHPGGPQK(Fitc)C-PL-MPEG (Cy5.5-CatK-PGC). The Cy5.5 molecules are in close proximity, which results in fluorescence quenching because of efficient fluorescence resonance energy transfer. The NIR fluorescence signal will increase when the Gly-Gly bond is cleaved by CatK, releasing Cy5.5-containing fragments. Cy5.5 has an absorbance maximum at 675 nm and an emission maximum at 694 nm with a high extinction coefficient of 250,000 M^-1^cm^-1^. Cy5.5-CatK-PGC is being developed for NIR fluorescence imaging of CatK proteolytic activity in tumors, atherosclerosis, myocardial infarction, and other diseases.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Poly-L-lysine+MPEG+synthesis)]

PL-MPEG was formed by a reaction of the hydroxysuccinimde ester of MPEG succinate to the NH_2_ group of PL (35.5 kDa) (14). The purified PL-MPEG had a calculated average molecular mass of 480 kDa as determined by elemental analysis. The PL-MPEG was then iodoacetylated by reaction with excess iodoacetic acid. GHPGGPQK(Fitc)C was coupled to the iodoacetylated PL-MPEG via a thiol-specific reaction at the C-terminal amino acid (C) (12). The resulting PGC was further modified with Cy5.5 hydroxysuccinimide ester via the free N-terminal amino acid (G) of the attached peptide. Cy5.5-CatK-PGC was purified by column chromatography. Each PL backbone contained an average of 92 MPEG molecules, 18 copies of CatK peptide, and 18 molecules of Cy5.5.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Poly-L-lysine+MPEG+and+in+vitro)]

Jaffer et al. (13) showed that Cy5.5-CatK-PGC (0.1 nM) was activated by the CatK enzyme (50 pmol) in a time-dependent manner with a 9-fold increase in NIR fluorescence signal after 15 h of incubation. Cy5.5-CatK-PGC was activated by CatK >2-fold versus with CatB and CatL, and >14-fold versus with MMP-2 and MMP-9. Furthermore, incubation of human carotid atheroma specimens with Cy5.5-CatK-PGC provided highest NIR fluorescence signal at 24 h with 127.0 ± 56.7 AU (P < 0.05), whereas the probe showed less signal with either a control Cy5.5 agent (36.0 ± 8.0 AU) or saline (9.5 ± 6.0 AU). The NIR fluorescence signal colocalized with immunoreactivity for CatK and CD68 (a macrophage marker) in the vicinity of macrophages.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Poly-L-lysine+MPEG+rodentia)]

Jaffer et al. (13) performed in vivo imaging of atherosclerosis in apolipoprotein E–deficient (apoE^-/-^) mice using intravital fluorescence microscopy after injection of 5 nmol Cy5.5-CatK-PGC. Increased fluorescence signal (174% increase; P < 0.05) could be detected in the aortic arch and root of the apoE^-/-^ mice 24 h after injection of the probe (target/background ratio 3.5 ± 1.4) compared with apoE^-/-^ mice injected with the control agent (target/background ratio 1.3 ± 0.2). Ex vivo imaging showed that the plaque NIR fluorescence signal intensity colocalized with immunoreactivity for CD68 in the vicinity of macrophages. No in vivo blocking or CatK inhibition experiments were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Poly-L-lysine+MPEG+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Poly-L-lysine+MPEG+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Poly-L-lysine+MPEG+human)]

No publication is currently available.

## NIH Support

U01 HL080731, R01-HL080472, P50-CA86355, R24-CA92782

## References

1 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
2 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
3 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
4 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
5 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
6 Keppler D., Sameni M., Moin K., Mikkelsen T., Diglio C.A., Sloane B.F. (1996). Tumor progression and angiogenesis: cathepsin B & Co. Biochem Cell Biol.
7 Liu J., Sukhova G.K., Sun J.S., Xu W.H., Libby P., Shi G.P. (2004). Lysosomal cysteine proteases in atherosclerosis. Arterioscler Thromb Vasc Biol.
8 Berchem G., Glondu M., Gleizes M., Brouillet J.P., Vignon F., Garcia M., Liaudet-Coopman E. (2002). Cathepsin-D affects multiple tumor progression steps in vivo: proliferation, angiogenesis and apoptosis. Oncogene.
9 Brix K., Dunkhorst A., Mayer K., Jordans S. (2007). and Cysteine cathepsins: Cellular roadmap to different functions. Biochimie.
10 Marecos E., Weissleder R., Bogdanov A. (1998). Antibody-mediated versus nontargeted delivery in a human small cell lung carcinoma model. Bioconjug Chem.
11 Weissleder R., Cheng H.C., Marecos E., Kwong K., Bogdanov A. (1998). Non-invasive in vivo mapping of tumour vascular and interstitial volume fractions. Eur J Cancer.
12 Lecaille F., Weidauer E., Juliano M.A., Bromme D., Lalmanach G. (2003). Probing cathepsin K activity with a selective substrate spanning its active site. Biochem J.
13 Jaffer F.A., Kim D.E., Quinti L., Tung C.H., Aikawa E., Pande A.N., Kohler R.H., Shi G.P., Libby P., Weissleder R. (2007). Optical visualization of cathepsin K activity in atherosclerosis with a novel, protease-activatable fluorescence sensor. Circulation.
14 Weissleder R., Tung C.H., Mahmood U., Bogdanov A. (1999). In vivo imaging of tumors with protease-activated near-infrared fluorescent probes. Nat Biotechnol.